# 1-(2’-Deoxy-2’-[^18^F]-fluoro-β-D-arabinofuranosyl)thymine

Chemical name: | 1-(2’-Deoxy-2’-[^18^F]fluoro-β-D-arabinofuranosyl)thymine
Abbreviated name: | [^18^F]FMAU
Synonym: | 2’-Deoxy-2’-[^18^F]fluoro-5-methyl-1-β-D-arabinofuranosyluracil; 1-(2’-deoxy-2’-[^18^F]fluoro-β-D-arabinofuranosyl)-5 methyluracil
Agent Category: | Compound
Target: | DNA
Target Category: | Incorporation into DNA
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU&WebEnv=0vHd3ETLPN9js1mOtFBfFbwDARincruHlBNNlBWjfRnIe7KeVe9lUjKtGwRySJD4LPw8_O1P75C9mz%407748428072881B60_0000SID&WebEnvRq=1)]

Cell proliferation and cell growth in various biological systems in an in vitro setting are routinely measured by the incorporation of radiolabeled (usually with radioactive C-14 or H-3) thymidine (TdR) because it is a necessary and exclusive component required for the synthesis of DNA in an organism (1). However, TdR was observed to be unsuitable for in vivo studies because it is easily catabolized by enzymes after administration and generated results that were complicated to interpret (2-4). Investigators initially developed a carbon (^11^C)-labeled TdR to study tumor growth with positron emission tomography (PET), but realized that the catabolic products of the labeled compound yielded low tumor/normal tissue contrast ratios (4). Therefore, to circumvent the catabolite issue observed with TdR, some investigators developed TdR analogs that were labeled with either radioactive fluorine (^18^F) or ^11^C, were not catabolized in vivo by virtue of the 2’-fluoro substitution, and could be used to monitor or image tumors or other rapidly proliferating tissue (3, 5, 6). Among the various TdR analogs, [^18^F]-3’-deoxy-3’-fluorothymidine ([^18^F]FLT) was used to study different cancers in the clinic. This compound is converted into a triphosphate by cytosolic thymidine kinase (TK_1_), is not incorporated into the DNA strand, and terminates elongation of the DNA chain (7). Because [^18^F]FLT is only phosphorylated by TK_1_ and is not incorporated into the DNA, the uptake of this radiochemical is considered only as an indicator of the TK_1_ enzyme activity. Moreover, the use of TK1 activity as a measure of DNA synthesis is not well established (8). In addition, [^18^F]FLT is known to produce high background in the liver, bone marrow, and the pelvis, so it is not considered to be a suitable agent to detect malignancies in these tissues or in this region of the body (9).

1-(2’-Deoxy-2’-fluoro-β-D-arabinofuranosyl)thymidine (FMAU) is another analog of TdR that was labeled with either ^18^F or ^11^C and used in vivo to investigate cell proliferation and tumor imaging (2, 10, 11). FMAU differs from TdR in that a hydrogen atom at the 2’ position of the deoxyarabinose sugar moiety in the molecule is substituted with fluorine, but both molecules possess the same biological properties (e.g., transport across the cell membrane, phosphorylation, and incorporation into cellular DNA) (2, 12). Also, compared to TdR, the clearance of [^11^C]FMAU from the blood was observed to be slower and showed a higher incorporation in tumors (12). However, the use of [^11^C]FMAU was limited by the short half-life of ^11^C, so an ^18^F-labeled version was produced to image cell proliferation and tumors in patients (10).

Because FMAU is a DNA synthesis inhibitor, it has been used as an antiviral agent and also as an antineoplastic agent for the treatment of cancers (13, 14). FMAU triphosphate was shown to inhibit the hepatitis B virus polymerase enzyme in a concentration-dependent manner, and it has been approved by the United States Food and Drug Administration for evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=FMAU) to treat this infection (14).

This chapter details the preclinical and clinical studies performed with [^18^F]FMAU. Studies performed with [^11^C]FMAU are presented in a separate chapter in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU+synthesis&WebEnv=0zRIUzECV7v4m50VlPy73YbwIWehkD0Xym_Ti-MIUyryiGHtpgd4rbA44LPfQUbxXXm8GrDUmAPqRz%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of [^18^F]FMAU was described by Alauddin et al. (15). The initial compound, 2-deoxy-2-[^18^F]fluoro-1,3,5-tri-O-benzoyl-a-D-arabinofuranose-2 was prepared by the modification of a previously published method (16). Briefly, aqueous [^18^F]-fluoride was added to a solution of tetrabutylammonium bicarbonate and evaporated azeotropically to dryness with acetonitrile at 80°C under a stream of argon. Subsequently, tetrabutylammonium [^18^F]-fluoride in dry acetonitrile was added to the dry residue, and the reaction mixture was heated at 80–82°C for 30 min. The mixture was then cooled to room temperature, passed through a Sep-Pak silica gel cartridge, and eluted with ethyl acetate. The solvent was then evaporated at 80°C under a stream of argon, and the product, a radiolabeled fluorosugar, was used for the next step without further purification.

The radiolabeled fluorosugar was dissolved in 1,2-dichloroethane under argon, and hydrogen bromide (HBr) in acetic acid (AcOH) was added to it. The reaction mixture was then heated for 10 min at 80–82°C and diluted with toluene. The HBr/AcOH solvent was evaporated under a stream of argon to obtain a dry, crude product, 1-bromo-2-deoxy-2-[^18^F]fluoro-3,5-di-O-benzoylarabinofuranose, which was used for the coupling experiment without purification.

A solution of freshly prepared 2,4-bis-O-(trimethylsilyl)thymine in 1,2-dichloroethane was added to 1-bromo-2-deoxy-2-[^18^F]fluoro-3,5-di-O-benzoylarabinofuranose, and the solution was heated at 97–100°C for 60 min. The reaction mixture was then cooled to room temperature and passed through a Sep-Pak silica gel cartridge. The column was eluted with 10% methanol in dichloromethane, and the solvent was evaporated at 100°C under a stream of argon to recover the crude product, 2’-deoxy-2’-[^18^F]fluoro-3’,5’-di-O-benzoyl-5-methyl-1-β/β-D-arabinofuranosyluracil.

The crude mixture of 2’-deoxy-2’-[^18^F]fluoro-3’,5’-di-O-benzoyl-5-methyl-1-β/β-D-arabinofuranosyluracil was dissolved in methanol, and a 1 M sodium methoxide solution in methanol was added. The mixture was then heated for 5 min at reflux, cooled, and neutralized with 2 N hydrochloric acid in methanol. The methanol was evaporated, and the remaining contents were diluted with acetonitrile/water and purified with high-performance liquid chromatography (HPLC) on a C18 reverse-phase column. The appropriate fractions were collected and evaporated to dryness. The pure product, [^18^F]FMAU, was dissolved again in saline, filter-sterilized, and analyzed with analytical HPLC.

The average radiochemical yield from this synthesis was reported to be 25% (n = 4) with a radiochemical purity of >99%. The synthesis time was 3.5–4.0 h from the end of bombardment, and the average specific activity of the product was reported to be 2,300 mCi/μmol (85 TBq/μmol) (15).

Mangner et al. (17) published another multi-step procedure for the synthesis of [^18^F]FMAU based on the procedure of Howell and colleagues (18, 19). Mangner et al. reported a decay-corrected radiochemical yield of 35–45%, and the radiochemical purity was routinely >98% (17). The synthesis time required was ~3 h, and the specific activity was >3 Ci/μmol (110 MBq/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU+in+vitro&WebEnv=0xIf2pdaG9HQ6cAInt403tfxsJvmo4Ztgl7wnQsJpnFMpJlv2iWg1uQNQjJxDl4K5I4gUbwUgATrR%407748428072881B60_0000SID&WebEnvRq=1)]

Using [^14^C]FMAU (available commercially) as a surrogate molecule, Alauddin et al. performed in vitro uptake studies of the radiochemical in herpes simplex virus 1 thymidine kinase (tk) gene–transduced MDA-MB-468 (http://www.biotech.ist.unige.it/cldb/cl4973.html) cells (tk-positive), a human breast cancer cell line (20). For this study, wild-type cells and vector-only–transduced cells (tk-negative) were used as controls. The tk-transduced cells consistently showed a 14–16-fold (P < 0.001) and a 146–233-fold higher (P < 0.001) incorporation of FMAU compared to the tk-negative and the wild-type cells, respectively. The tk-positive cells had a 2.7–7.1-fold higher and the tk-negative cells had a 1.5–3.0-fold higher incorporation of labeled FMAU compared to the wild-type cells. In all three cell types, ~95% of the total radioactivity was detected in the DNA (20). No competition binding studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU+rodentia&WebEnv=04IJhD8kEdF1DfTqsJo0h_239lJka1hvg2ZHPuwBjmVQvGLE9yfKOSM87_Zn_aMdWY1EZ-BJrATeR%407748428072881B60_0000SID&WebEnvRq=1)]

The uptake of [^14^C]FMAU was also investigated in nude mice (n = 5) bearing tk-positive and tk-negative tumors derived from the MDA-MB-468 cells described above (20). The ratio of [^14^C]FMAU uptake between the tk-positive and the tk-negative tumors 1 h after administration was 3.7 (P < 0.001), and the tk-positive tumor/blood ratio was 4.3 (P < 0.001). At 2 h after administration, the tk-positive/tk-negative tumor cell ratio was 5.5 (P < 0.001), and the tk-positive tumor/blood ratio was 13.4 (P < 0.001). The [^14^C]FMAU uptake ratio between the tk-positive tumor and other organs was reported to be in the range of 5.5–15.6.

Imaging studies with [^18^F]FMAU in the five nude, tumor-bearing mice tumors described above showed that the label accumulated primarily in the tk-positive tumors and had a biodistribution that was similar to the ^14^C homolog (20). However, with this compound a high accumulation was noted in the intestine because it obscured the visibility of a tk-positive tumor on the right flank of the animal. No competition binding studies were reported with these animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU+nonprimate+mammals&WebEnv=0gZ_hXyeHrJNGgnJLyWmGapPIQnMzYLa97ymASrNTMhLqdT--CVjnRN3NGZqLzBu3NcBLLQeLQEbs%407748428072881B60_0000SID&WebEnvRq=1)]

Sun et al. investigated the biodistribution of [^18^F]FMAU in dogs (n = 5) (21).The animals were injected with the tracer, and imaging studies were performed up to 2.5 h after administration. At the end of each study, select tissue was removed to determine the radioactivity that accumulated. Incorporated radioactivity in DNA was also determined after extraction of the macromolecule. On imaging and tissue analysis, an increased accumulation of the label was apparent in the lymph nodes, stomach, small intestines, and the bone marrow, which corresponded with the degree of cell proliferation observed in these tissues. The highly proliferative tissues, the intestines and the bone marrow, were reported to have an accumulation of ~88% and ~65% of the total activity in DNA, respectively (21). The tissue/muscle ratio in the non-proliferative organs such as the lungs, heart, liver, and the kidneys was 1.0, and only ~10% of the total activity was detected in the DNA of these organs.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU+nonhuman+primates&WebEnv=0jCLW2EHyXjk88dzfAT-XdXVnW64ShPAtTQu0MWPdZOgrtay01JRyKHch3mPy5YyWPr0vokfUkFNK%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMAU+humans&WebEnv=0Kl4mgVbN1d-aB3H_GlhJ8lMM5hLzgfivWm3cMdSZWu2xNyleeiTj0wVLFukmFK4yI93gH1AtAmnE%407748428072881B60_0000SID&WebEnvRq=1)]

A pilot study was conducted to evaluate [^18^F]FMAU for DNA synthesis in tumors and to determine its biodistribution in cancer patients (10). The radiopharmaceutical was used to image patients (n = 14) with either prostate, brain, colorectal, lung, or breast cancer. Dynamic PET images were obtained 60 min after the administration of [^18^F]FMAU, and metabolite clearance was also determined with HPLC in the blood and urine. The normal bone marrow was reported to have a mean standardized uptake value (SUV) of 0.7, and the tumor SUVs were 2.19, 1.28, 2.21, and 2.27–4.42 for lesions in the breast, brain, lungs, and prostate. High SUVs were observed in the liver (SUV 10.07–20.88) and the kidneys (SUV 7.18–15.66), probably because of metabolism and excretion in these organs. Compared to these organs, the bladder had a low mean SUV of 2.03. The investigators reported that 95% of the activity was cleared from blood circulation within 10 min, and 70% of the activity in the urine was intact [^18^F]FMAU at 60 min after administration (10).

Tehrani et al. investigated the uptake of [^18^F]FMAU in patients with brain (n = 4) and prostate (n = 6) cancers to determine the easiest approach for image acquisition and analysis (11). The investigators obtained 60-minute dynamic images and determined the mean and maximum SUVs for the tumors. The mean tumor SUVs obtained between 5 and 11 min were reported to correlate with the values obtained between 30 and 60 min (r^2^ = 0.92; P < 0.0001), and the maximum SUVs also showed a similar correlation. The investigators cautioned that, although this radiopharmaceutical was suitable to obtain usable images of the brain and prostate tumors at 11 min after administration of [^18^F]FMAU, the study was performed with a small number of patients which means that it would be necessary to perform this study in a larger patient population with a wide range of tumors to generalize this procedure.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the studies presented in this chapter were funded by NCI grants CA 83131, CA 82645, and CA 72896.

## References

1 Shields A.F. (2006). Positron emission tomography measurement of tumor metabolism and growth: its expanding role in oncology. Mol Imaging Biol.
2 Conti P.S., Hilton J., Wong D.F., Alauddin M.M., Dannals R.F., Ravert H.T., Wilson A.A., Anderson J.H. (1994). High performance liquid chromatography of carbon-11 labeled thymidine and its major catabolites for clinical PET studies. Nucl Med Biol.
3 Lu L., Samuelsson L., Bergstrom M., Sato K., Fasth K.J., Langstrom B. (2002). Rat studies comparing 11C-FMAU, 18F-FLT, and 76Br-BFU as proliferation markers. J Nucl Med.
4 Mankoff D.A., Shields A.F., Link J.M., Graham M.M., Muzi M., Peterson L.M., Eary J.F., Krohn K.A. (1999). Kinetic analysis of 2-[11C]thymidine PET imaging studies: validation studies. J Nucl Med.
5 Grierson J.R., Shields A.F., Zheng M., Kozawa S.M., Courter J.H. (1995). Radiosyntheses of labeled beta-pseudothymidine ([C-11]- and [H-3]methyl) and its biodistribution and metabolism in normal and tumored mice. Nucl Med Biol.
6 Krohn K.A., Mankoff D.A., Eary J.F. (2001). Imaging cellular proliferation as a measure of response to therapy. J Clin Pharmacol.
7 Reske S.N., Deisenhofer S. (2006). Is 3'-deoxy-3'-(18)F-fluorothymidine a better marker for tumour response than (18)F-fluorodeoxyglucose?. Eur J Nucl Med Mol Imaging.
8 Rasey J.S., Grierson J.R., Wiens L.W., Kolb P.D., Schwartz J.L. (2002). Validation of FLT uptake as a measure of thymidine kinase-1 activity in A549 carcinoma cells. J Nucl Med.
9 Groves A.M., Win T., Haim S.B., Ell P.J. (2007). Non-[18F]FDG PET in clinical oncology. Lancet Oncol.
10 Sun H., Sloan A., Mangner T.J., Vaishampayan U., Muzik O., Collins J.M., Douglas K., Shields A.F. (2005). Imaging DNA synthesis with [18F]FMAU and positron emission tomography in patients with cancer. Eur J Nucl Med Mol Imaging.
11 Tehrani O.S., Muzik O., Heilbrun L.K., Douglas K.A., Lawhorn-Crews J.M., Sun H., Mangner T.J., Shields A.F. (2007). Tumor imaging using 1-(2'-deoxy-2'-18F-fluoro-beta-D-arabinofuranosyl)thymine and PET. J Nucl Med.
12 Bading J.R., Shahinian A.H., Vail A., Bathija P., Koszalka G.W., Koda R.T., Alauddin M.M., Fissekis J.D., Conti P.S. (2004). Pharmacokinetics of the thymidine analog 2'-fluoro-5-methyl-1-beta-D-arabinofuranosyluracil (FMAU) in tumor-bearing rats. Nucl Med Biol.
13 Fanucchi M.P., Leyland-Jones B., Young C.W., Burchenal J.H., Watanabe K.A., Fox J.J. (1985). Phase I trial of 1-(2'-deoxy-2'-fluoro-1-beta-D-arabinofuranosyl)-5-methyluracil (FMAU). Cancer Treat Rep.
14 Korba B.E., Furman P.A., Otto M.J. (2006). Clevudine: a potent inhibitor of hepatitis B virus in vitro and in vivo. Expert Rev Anti Infect Ther.
15 Alauddin M.M., Conti P.S., Fissekis J.D. (2002). Synthesis of [18F]-labeled 2'-deoxy-2'-fluoro-5-methyl-1-beta-D-arabinofuranosyluracil. J Label Compd Radiopharm.
16 Alauddin M.M., Conti P.S., Mathew T., Fissekis J.D., Prakash G.K.S., Watanabe K.A. (2000). Stereospecific fluorination of 1,3,5-tri-O-benzoyl-α--ribofuranose-2-sulfonate esters: preparation of a versatile intermediate for synthesis of 2'-[18F]-fluoro-arabinonucleosides. Journal of Fluorine Chemistry.
17 Mangner T.J., Klecker R.W., Anderson L., Shields A.F. (2003). Synthesis of 2'-deoxy-2'-[18F]fluoro-beta-D-arabinofuranosyl nucleosides, [18F]FAU, [18F]FMAU, [18F]FBAU and [18F]FIAU, as potential PET agents for imaging cellular proliferation. Synthesis of [18F]labelled FAU, FMAU, FBAU, FIAU. Nucl Med Biol.
18 Howell H.G., Brodfuehrer P.R., Brundidge S.P., Benigni D.A., Sapino C. (1988). Antiviral nucleosides. A stereospecific, total synthesis of 2'-fluoro-2'-deoxy-beta-D-arabinofuranosyl nucleoside. J Org Chem.
19 Tann C.H., Brodfuehrer P.R., Brundidge S.P., Sapino C., Howell H.G. (1985). Fluorocarbohydrates in synthesis. An efficient synthesis of 1-(2-deoxy-2-fluoro-beta-D-arabinofuranosyl)-5-iodouracil (b-FIAU) and 1-(2-deoxy-2-fluoro-beta-D-arabinofuranosyl)thymine (b-FMAU). J Org Chem.
20 Alauddin M.M., Shahinian A., Gordon E.M., Conti P.S. (2004). Direct comparison of radiolabeled probes FMAU, FHBG, and FHPG as PET imaging agents for HSV1-tk expression in a human breast cancer model. Mol Imaging.
21 Sun H., Mangner T.J., Collins J.M., Muzik O., Douglas K., Shields A.F. (2005). Imaging DNA synthesis in vivo with 18F-FMAU and PET. J Nucl Med.